# ^68^Ga-1,4,7-Triazacyclononane-1,4,7-triacetic acid-c(RGDfK)-human serum albumin-tissue inhibitor of matrix metalloproteinase 2 fusion protein

Chemical name: | ^68^Ga-1,4,7-Triazacyclononane-1,4,7-triacetic acid-c(RGDfK)-human serum albumin-tissue inhibitor of matrix metalloproteinase 2 fusion protein
Abbreviated name: | ^68^Ga-NOTA-RGD-HSA-TIMP2
Synonym:
Agent category: | Protein
Target: | α_v_β_3_ integrin receptor
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal/contrast: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RGD-HSA-TIMP-2)]

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degrading the basement membrane and ECM (3).

Several families of MMPs are involved in atherogenesis, myocardial infarction, angiogenesis, and tumor invasion and metastases (4-7). MMP expression is highly regulated in normal cells, such as trophoblasts, osteoclasts, neutrophils, and macrophages. Elevated levels of MMPs have been found in tumors associated with a poor prognosis for cancer patients (8). There are four members of endogenous tissue inhibitors of metalloproteinases (TIMPs), which regulate the activity of MMPs leading to inhibition of tumor growth and metastasis (9, 10). TIMP-2 (TIMP2) is a bifunctional inhibitor of angiogenesis by inhibition of proteinase activity of MMPs and endothelial cell proliferation via binding to α_3_β_1_ (the N-terminal domain) and by MMP-independent anti-angiogenic activity (the C-terminal domain) (11, 12). Kang et al. (13) fused the N-terminal domain of TIMP2 to the C-terminus of human serum albumin (HSA) to form HSA/TIMP2 fusion protein (HSA-TIMP2), which is readily secreted by the transfected yeast Saccharomyces cerevisiae. HSA-TIMP2 retains its anti-angiogenic activity at the C-terminal domain with little MMP inhibitory activity at the N-terminal domain. Lee et al. (14) have evaluated Cy5.5-HSA/TIMP2 (Cy5.5-HSA-TIMP2) for in vivo near-infrared (NIR) fluorescence imaging of rat prostate MLL tumors in nude mice showing maximum tumor accumulation at 2 d after injection.

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (15). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (16-21). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. The peptide sequence Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. The α_v_β_3_ antagonists are being studied as anti-tumor and anti-angiogenic agents (18, 22, 23). Various radiolabeled RGD peptides (antagonists) have been introduced for imaging of tumors and tumor angiogenesis (24). Choi et al. (25) conjugated multiple c(RGDfK) peptides to HSA-TIMP2 to enhance the binding capacity of the protein (RGD-HSA-TIMP2) to tumors and their vasculatures. ^68^Ga-NOTA-RGD-HSA-TIMP2 and ^68^Ga-NOTA-HSA-TIMP2 have been studied as potential positron emission tomography (PET) probes for imaging α_v_β_3_ integrin receptors in nude mice bearing human glioblastoma U87MG tumors.

### Related Resource Links:

- Chapters in MICAD (MMP (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=matrix+metalloproteinases+AND+micad%5Bbook%5D), TIMP (http://www.ncbi.nlm.nih.gov/books?term=TIMP%20AND%20micad%5Bbook%5D), RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D))
- Gene information in NCBI (TIMP2 (http://www.ncbi.nlm.nih.gov/gene/7077), HSA (http://www.ncbi.nlm.nih.gov/gene/213), α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), α_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3675), β_1_ integrin (http://www.ncbi.nlm.nih.gov/gene/3688), β_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3690))
- Articles in Online Mendelian Inheritance in Man (OMIM) (TIMP2 (http://omim.org/entry/188825), HSA (http://omim.org/entry/103600), α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), α_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/605025), β_1_ integrin (http://www.ncbi.nlm.nih.gov/omim/135630), β_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/173470))
- Clinical trials (TIMP (http://www.clinicaltrials.gov/ct2/results?term=TIMP), RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD))
- Drug information in FDA (TIMP (http://google2.fda.gov/search?q=TIMP&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*), RGD (http://google2.fda.gov/search?q=RGD&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HSA-TIMP-2)]

HSA-TIMP2 and c[RGDfK(COCH_2_SH)] was incubated with N-succinimidyl iodoacetate to form a thioether linkage between the RGD peptide and HSA-TIMP2 protein (25). RGD-HSA-TIMP2 was purified with column chromatography. The molecular weights of RGD-HSA-TIMP2 and HSA-TIMP2 were calculated to be 88.42 kDa and 92.78 kDa with mass spectroscopy, respectively. There were 6 RGD molecules per RGD-HSA-TIMP2. Addition of NOTA groups to RGD-HSA-TIMP2 and HSA-TIMP2 was performed by mixing 0.05 µmol protein with 2.2 µmol SCN-Bz-NOTA in 0.1 M sodium carbonate buffer (pH 9.5) for 20 h at room temperature. The NOTA-conjugated proteins were purified with column chromatography. The number of NOTA moieties per NOTA-RGD-HSA-TIMP2 and NOTA-HSA-TIMP2 were calculated to be 6.6 and 5.1, respectively. For ^68^Ga labeling, a solution of 74 MBq (2 mCi) ^68^GaCl_3_ and NOTA-RGD-HSA-TIMP2 or NOTA-HSA-TIMP2 was incubated for 20 min at room temperature. ^68^Ga-NOTA-RGD-HSA-TIMP2 and ^68^Ga-NOTA-HSA-TIMP2 was purified with column chromatography, with yields of 30%–35% and total synthesis time of 30 min. Their specific activities and radiochemical purities were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HSA-TIMP-2%20and%20in%20vitro)]

Flow cytometry analysis showed that 45% and 91% of U89MG cells were positive after incubation with HSA-TIMP2-FITC and RGD-HSA-TIMP2-FITC for 24 h at 4°C (25), respectively. Confocal microscopy showed internalization of fluorescence activity inside the cells incubated with 1.6 nM RGD-HSA-TIMP2-FITC for 3 h at 37°C but not with HSA-TIMP2-FITC. No blocking studies were performed with unlabeled RGD-HSA-TIMP2.

In vitro cell viability of U87MG was assessed after incubation with various concentrations (0.11–3.2 nM) of RGD, HSA-TIMP2, and RGD-HSA-TIMP2 for 24 h at 37°C (25). The cell viability values with 3.2 nM RGD, HSA-TIMP2, and RGD-HSA-TIMP2 were 92.5 ± 4.0%, 73.5 ± 7.9% (P < 0.05 versus RGD), and 66.7 ± 0.6% (P < 0.01 versus RGD), respectively.

Cellular accumulation of ^68^Ga-NOTA-RGD-HSA-TIMP2 and ^68^Ga-NOTA-HSA-TIMP2 was compared in human glioblastoma U87MG (positive for α_v_β_3_ integrin) and rat glioblastoma C6 (negative for α_v_β_3_ integrin) cells in culture (25). The radioactivity levels of ^68^Ga-NOTA-HSA-TIMP2 were low in C6 (0.23 ± 0.01% incubation dose (ID)) and U87MG (0.49 ± 0.01% ID) cells at 3 h after incubation. However, the radioactivity level of ^68^Ga-NOTA-RGD-HSA-TIMP2 was higher in U87MG (3.87 ± 0.49% ID) than in C6 (0.71 ± 0.01% ID) cells. Co-incubation of ^68^Ga-NOTA-RGD-HSA-TIMP2 with excess c(RGDyK) significant inhibited the radioactivity level in U89MG cells by 70% (P < 0.01). No affinity constants were reported for the three constructs.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HSA-TIMP-2%20and%20rodentia)]

Choi et al. (25) performed ex vivo biodistribution studies of 3.7 MBq (0.01 mCi) ^68^Ga-NOTA-RGD-HSA-TIMP2 and ^68^Ga-NOTA-HSA-TIMP2 in nude mice (n = 3/group) bearing U87MG xenografts at 3 h after injection. The tumor accumulation of radioactivity was 1.1 ± 0.2% ID/g and 0.4 ± 0.1% ID/g for ^68^Ga-NOTA-RGD-HSA-TIMP2 and ^68^Ga-NOTA-HSA-TIMP2 (P < 0.01), respectively. The organ with the highest accumulation was the liver for both radiolabeled proteins with ~40% ID/g. The kidney and spleen accumulation values were 3% ID/g and 8% ID/g, respectively. The blood concentrations were approximately four-fold higher than the tumor accumulation, suggesting that more time is needed to have optimal accumulation in the tumors. No blocking studies were performed.

Choi et al. (25) performed whole-body PET/CT imaging in nude mice (the number of mice was not reported) bearing U87MG tumors at 1 h and 3 h after intravenous injection of 7.2 MBq (0.2 mCi) ^68^Ga-NOTA-RGD-HSA-TIMP2 and ^68^Ga-NOTA-HSA-TIMP2. Little tumor accumulation of ^68^Ga-NOTA-HSA-TIMP2 was observed at 1 h (0.56 ± 0.08% ID/g) and 3 h (0.69 ± 0.09% ID/g). The tumor accumulation of ^68^Ga-NOTA-RGD-HSA-TIMP2 was 0.77 ± 0.07% ID/g and 1.95 ± 0.50% ID/g at 1 h and 3 h, respectively. High liver accumulation was observed with both tracers. Immunofluorescence staining of tumor tissue sections showed an increase in CD31 (endothelial cell biomarker) expression in the tumor tissue. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HSA-TIMP-2%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HSA-TIMP-2%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HSA-TIMP-2%20and%20human)]

No publication is currently available.

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
4 Keppler D., Sameni M., Moin K., Mikkelsen T., Diglio C.A., Sloane B.F. (1996). Tumor progression and angiogenesis: cathepsin B & Co. Biochem Cell Biol.
5 Liu J., Sukhova G.K., Sun J.S., Xu W.H., Libby P., Shi G.P. (2004). Lysosomal cysteine proteases in atherosclerosis. Arterioscler Thromb Vasc Biol.
6 Berchem G., Glondu M., Gleizes M., Brouillet J.P., Vignon F., Garcia M., Liaudet-Coopman E. (2002). Cathepsin-D affects multiple tumor progression steps in vivo: proliferation, angiogenesis and apoptosis. Oncogene.
7 Brix, K., A. Dunkhorst, K. Mayer, and S. Jordans, Cysteine cathepsins: Cellular roadmap to different functions. Biochimie, 2007
8 Deryugina E.I., Quigley J.P. (2006). Matrix metalloproteinases and tumor metastasis. Cancer Metastasis Rev.
9 Baker A.H., Edwards D.R., Murphy G. (2002). Metalloproteinase inhibitors: biological actions and therapeutic opportunities. J Cell Sci.
10 Jiang Y., Goldberg I.D., Shi Y.E. (2002). Complex roles of tissue inhibitors of metalloproteinases in cancer. Oncogene.
11 Fernandez C.A., Butterfield C., Jackson G., Moses M.A. (2003). Structural and functional uncoupling of the enzymatic and angiogenic inhibitory activities of tissue inhibitor of metalloproteinase-2 (TIMP-2): loop 6 is a novel angiogenesis inhibitor. J Biol Chem.
12 Seo D.W., Li H., Guedez L., Wingfield P.T., Diaz T., Salloum R., Wei B.Y., Stetler-Stevenson W.G. (2003). TIMP-2 mediated inhibition of angiogenesis: an MMP-independent mechanism. Cell.
13 Kang W.K., Park E.K., Lee H.S., Park B.Y., Chang J.Y., Kim M.Y., Kang H.A., Kim J.Y. (2007). A biologically active angiogenesis inhibitor, human serum albumin-TIMP-2 fusion protein, secreted from Saccharomyces cerevisiae. Protein Expr Purif.
14 Lee M.S., Kim Y.H., Kim Y.J., Kwon S.H., Bang J.K., Lee S.M., Song Y.S., Hahm D.H., Shim I., Han D., Her S. (2011). Pharmacokinetics and biodistribution of human serum albumin-TIMP-2 fusion protein using near-infrared optical imaging. J Pharm Pharm Sci.
15 Hynes R.O. (2002). A reevaluation of integrins as regulators of angiogenesis. Nat Med.
16 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
17 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
18 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
19 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
20 Varner J.A., Cheresh D.A. (1996). Integrins and cancer. Curr Opin Cell Biol.
21 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
22 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
23 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
24 Haubner R., Beer A.J., Wang H., Chen X. (2010). Positron emission tomography tracers for imaging angiogenesis. Eur J Nucl Med Mol Imaging.
25 Choi N., Kim S.M., Hong K.S., Cho G., Cho J.H., Lee C., Ryu E.K. (2011). The use of the fusion protein RGD-HSA-TIMP2 as a tumor targeting imaging probe for SPECT and PET. Biomaterials.